# ^111^In-Diethylenetriamine pentaacetic acid-QKYGNQWAVGHLM-NH_2_

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-QKYGNQWAVGHLM-NH_2_
Abbreviated name: | ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5bDTPA1-Lys3,%20Tyr4%5d-BN)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptor (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system and the gastrointestinal system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on central nervous system and gastrointestinal tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Prostate cancer is the third most common type of cancer in men in the United States. GRPR is overexpressed on human androgen-independent prostate PC-3 cancer cells. Ho et al. (7) radiolabeled diethylenetriamine pentaacetic acid-QKYGNQWAVGHLM-NH_2_ ([DTPA^1^-Lys^3^,Tyr^4^]-BN) with ^111^In. ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN has been evaluated as a single-photon emission computed tomography imaging agent of GRPR in nude mice bearing human PC-3 prostate cancer cells.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=BBN%20OR%20BN+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad) this link didn’t work on my MAC using Safari.
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=GRPR)
- Clinical trials (Bombesin (http://www.clinicaltrials.gov/ct2/results?term=bombesin))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5bDTPA1-Lys3,%20Tyr4%5d-BN+synthesis)]

[DTPA^1^-Lys^3^,Tyr^4^]-BN was prepared with solid-phase peptide synthesis (7). A mixture of [DTPA^1^-Lys^3^,Tyr^4^]-BN (0.525 nmol) and ^111^InCl_3_ (105 MBq (2.84 mCi)) was allowed to react for 10 min at 25°C. The product, ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN, was obtained with a yield of 97% and a radiochemical purity of >97%. The specific activity of ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN was 200 GBq/µmol (5.4 Ci/µmol). ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN was relatively stable in saline (99% intact), human plasma (83% intact), and rat plasma (76% intact) after 4 h of incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5bDTPA1-Lys3,%20Tyr4%5d-BN+in+vitro)]

Ho et al. (7) performed in vitro inhibition studies of [DTPA^1^-Lys^3^,Tyr^4^]-BN and BN using recombinant human BB2 receptor with ^125^I-Tyr^4^-BN. The 50% inhibition concentration (IC_50_) values for [DTPA^1^-Lys^3^,Tyr^4^]-BN and BN were 1.05 ± 0.46 nM and 0.05 ± 0.02 nM, respectively. The K_d_ and B_max_ values of ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN using PC-3 cells were determined to be 22.9 ± 6.8 nM and 880 fmol (~5 × 10^5^ receptor sites) per 10^6^ cells, respectively. PC-3 cells exhibited 26% uptake of the incubation dose of ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN within 60 min of incubation at 37°C, and 60% of radioactivity remained internalized after 120 min incubation in fresh medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5bDTPA1-Lys3,%20Tyr4%5d-BN+%20rodentia)]

Ho et al. (7) performed ex vivo biodistribution studies of 0.37 MBq (10 μCi) ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN in mice (n = 4–5/group) bearing PC-3 xenografts at 1, 4, 8, 24, and 48 h after injection. Tumor accumulation levels at these time points were 1.93 ± 0.25%, 1.60 ± 0.21%, 2.48 ± 0.48%, 1.23 ± 0.19%, and 0.93 ± 0.16% injected dose per gram (ID/g). The tumor/muscle ratio of 5.4 peaked at 8 h and decreased to 1.29 at 48 h. Pretreatment with excess [DTPA^1^-Lys^3^,Tyr^4^]-BN (1.05 nmol/mouse) inhibited accumulation in the tumor by 51% at 4 h and 66% at 24 h after injection, whereas accumulation in the pancreas was inhibited by 81% and 84%, respectively. The intestines also showed >50% inhibition at these time points. The organ with the highest uptake at 8 h after injection was the pancreas (32% ID/g), followed by the kidney (22% ID/g), adrenal (8% ID/g), small intestine (8% ID/g), and large intestine (7% ID/g). The heart, lung, stomach, muscle, bone, brain, and blood exhibited little accumulation of radioactivity at 8–48 h after injection.

Positron emission tomography imaging in nude mice (n = 4) bearing PC-3 xenografts was performed with 10 MBq (0.27 mCi) ^111^In-[DTPA^1^-Lys^3^,Tyr^4^]-BN at 1, 4, 8, 24, and 48 h after injection. The tumors were clearly visualized, as were the pancreas, intestines, and kidneys. Tumor standard uptake values at these time points were 1.60 ± 0.62, 1.62 ± 0.46, 2.48 ± 0.48, 1.47 ± 0.44, and 1.50 ± 0.49, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5bDTPA1-Lys3,%20Tyr4%5d-BN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5bDTPA1-Lys3,%20Tyr4%5d-BN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5bDTPA1-Lys3,%20Tyr4%5d-BN+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Ho C.L., Chen L.C., Lee W.C., Chiu S.P., Hsu W.C., Wu Y.H., Yeh C.H., Stabin M.G., Jan M.L., Lin W.J., Lee T.W., Chang C.H. (2009). Receptor-binding, biodistribution, dosimetry, and micro-SPECT/CT imaging of 111In-[DTPA(1), Lys(3), Tyr(4)]-bombesin analog in human prostate tumor-bearing mice. Cancer Biother Radiopharm.